# 3-Fluoromethyl-N-[^11^C]methyl-4-phenyl-N-(phenylmethyl)quinoline-2-carboxamide

Chemical name: | 3-Fluoromethyl-N-[^11^C]methyl-4-phenyl-N-(phenylmethyl)quinoline-2-carboxamide
Abbreviated name: | [^11^C]PBR6a
Synonym:
Agent category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR), also known as translocator protein (TSPO)
Target category: | Receptor
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+AND+6a)]

Benzodiazepines are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as the central benzodiazepine receptor (CBR) and the peripheral benzodiazepine receptor (PBR). The CBR is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the PBR is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBR than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBR (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage that accompanies several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo by positron emission tomography (PET) using 1-(2-chlorophenyl)-N-[^11^C]methyl-N-(1-methylpropyl)-3-isoquinoline carboxamide ([^11^C]PK11195), an isoquinoline carboxamide with specific PBR-antagonistic activity. [^11^C]PK11195 is being developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (8, 9). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than did PK11195 (8, 9). Therefore, both compounds are able to cross the normal cell membrane to reach the mitochondrial receptor sites. N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106) and [^11^C]DAA1106 have been developed as potential PET probes with highly selective and specific binding to PBR. In this chapter, 3-Fluoromethyl-N-[^11^C]methyl-4-phenyl-N-(phenylmethyl)quinoline-2-carboxamide ([^11^C]PBR6a) with a 2-quinolinecarboxamide structure has been developed to image PBR in the peripheral tissues, such as the heart, lung, kidney and spleen.

### Related Resource Links:

- Chapters in MICAD (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PBR%5BAll+Fields%5D+AND+micad%5Bbook%5D))
- Gene information in NCBI (PBR (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=706%5Buid%5D))
- Articles in OMIM (PBR (http://www.ncbi.nlm.nih.gov/entrez/dispomim.cgi?id=109610))
- Clinical trials (PBR (http://www.clinicaltrials.gov/ct2/results?term=pk11195+OR+PBR))
- Drug information in FDA (PBR (http://google2.fda.gov/search?q=Peripheral-type+benzodiazepine+receptor+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=5&y=5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+AND+6a+synthesis)]

In the report by Cappelli et al. (10), [^11^C]PBR6a was synthesized by ^11^C-methylation of the N-desmethyl precursor with ^11^C-labeled iodomethane in the presence of tetrabutylammonium hydroxide. [^11^C]PBR6a was purified by high-performance liquid chromatography with a 35–40% decay-corrected radiochemical yield. The specific activity was 55.5 GBq/μmol (1.5 Ci/μmol) at the end of synthesis with >99% radiochemical purity. Total synthesis time was 35 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+AND+6a+in+vitro)]

In vitro [^3^H]PK11195 PBR-binding to rat cortical membranes showed that BR6a had an inhibition concentration (IC_50_) value of 0.11 ± 0.02 nM (10). BR6a was ~20 times more potent than PK11195 (IC_50_ = 2.5 ± 0.4 nM).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+6a+rodentia)]

Cappelli et al. (10) reported biodistribution studies of [^11^C]PBR6a in rats that showed high accumulation of radioactivity in the lung (1.023% injected dose (ID)/g), followed by the adrenal gland (0.523% ID/g), heart (0.489% ID/g), spleen (0.487% ID/g), and kidney (0.358% ID/g) at 30 min after injection of [^11^C]PBR6a. The level of radioactivity was low in the brain (0.039% ID/g) and blood (0.020% ID/g). Pretreatment with PK11195 (5 mg/kg) decreased the accumulation in the heart, kidney, spleen, stomach, and lung by >74% but had no effect in the adrenal gland, blood, and brain at 30 min after injection. PET imaging in mice confirmed high levels of radioactivity in the lung, kidney, liver, heart, and spleen at 10–20 min after injection. Co-injection of PK11195 clearly reduced radioactivity in the lung, heart, and spleen, but not in the kidney or liver.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+6a+(dog+or+pig+or+sheep+or+rabbit))]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+6a+(primate+not+human))]

No publications are currently available.

## Human Studies

[Pub Med (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=pbr+6a+human)]

No publications are currently available.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Cappelli A., Matarrese M., Moresco R.M., Valenti S., Anzini M., Vomero S., Turolla E.A., Belloli S., Simonelli P., Filannino M.A., Lecchi M., Fazio F. (2006). Synthesis, labeling, and biological evaluation of halogenated 2-quinolinecarboxamides as potential radioligands for the visualization of peripheral benzodiazepine receptors. Bioorg Med Chem.